# 2-[^18^F]Fluoro-3-[2-((S)-3-pyrrolinyl)methoxy]pyridine

Chemical name: | 2-[^18^F]Fluoro-3-[2-((S)-3-pyrrolinyl)methoxy]pyridine
Abbreviated name:
Synonym: | [^18^F]Nifene
Agent Category: | Compound
Target: | α4β2 nicotinic acetylcholine receptor (nAChR)
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20nifene%5BAll%20Fields%5D)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2–α10) and four subtypes of structural β (β2–β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning, memory, and control of movement in normal subjects. Dysfunction of nAChRs has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction.

2-[^18^F]Fluoro-A-85380 (2-[^18^F]FA) and 6-[^18^F]FA have been evaluated as positron emission tomography (PET) agents for the non-invasive study of nAChRs in humans (4, 5). However, prolonged imaging times (2–4 h) are required for reliable quantification because of their slow kinetics. 2-Fluoro-3-[2-((S)-3-pyrrolinyl)methoxy]pyridine (nifene) is a highly potent and selective nAChR agonist with subnanomolar affinity (6). [^18^F]Nifene is being developed as a PET agent with faster kinetics than 2-[^18^F]FA and 6-[^18^F]FA for the non-invasive study of nAChRs in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20nifene%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Pichika et al. (6) reported synthesis of [^18^F]nifene by a two-step reaction consisting of standard ^18^F-nucleophilic fluorination of 2-nitro-3-[2-((S)-N-tert-butoxycarbonyl-3-pyrroline)methoxy]pyridine and acidic deprotection of the product. An average radiochemical yield was 40–50%, with a total synthesis time of 150 min. Specific activities were 37–186 GBq/μmol (1–5 Ci/μmol) at end of synthesis with a radiochemical purity of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20in%20vitro)]

Pichika et al. (6) reported that nifene, nifrolidine, and nicotine had respective K_i_ values of 0.50 ± 0.14, 0.80 ± 0.11, and 1.68 ± 0.28 nM in [^3^H]cytosine (α4β2 nicotinic acetylcholine receptor) binding assays using rat brain membranes. In vitro autoradiography studies of rat brain slices indicated selective binding of [^18^F]nifene to anteroventral thalamic (AVT) nucleus > thalamus > subiculum > striatum > cortex > cerebellum, consistent with α4β2 receptor distribution. The ratios of brain regions to cerebellum for AVT, thalamus, subiculum, striatum, and cortex were in the range of 13-19, 10-12, 7-8, 5, and 4, respectively. Nicotine blocked 60% (10 nM) and >95% (300 μM) of [^18^F]nifene-specific binding across the brain regions.

Easwaramoorthy et al. (7) estimated α4β2 receptor occupancy by acetylcholine using in vitro [^18^F]nifene autoradiography studies of rat brain slices in the presence of acetylcholinesterase inhibitors, physostigmine (PHY) and galanthamine (GAL). PHY (0.2-20 μM), GAL (0.4-4 μM) or acetylcholine (100 nM) alone had little effect on the [^18^F]nifene binding to AVT, thalamus, subiculum, striatum, and cortex. The combination of PHY (20 μM) and acetylcholine (100 nM) or GAL (4 μM) and acetylcholine (100 nM) exhibited 63-70% and 10-20% acetylcholine receptor occupancy, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20%28primate%20not%20human%29)]

A biodistribution PET study performed by Pichika et al. (6) in one anesthetized male rhesus monkey injected with 130 MBq (3.5 mCi) [^18^F]nifene showed rapid accumulation of radioactivity in the brain. PET study showed selective maximal uptake in the regions of the thalamus, lateral geniculate, cingulate gyrus, and temporal cortex including the subiculum. The cerebellum showed lower binding than the other brain regions. The thalamus/cerebellum ratio peaked at a value of 2.2 30–35 min after injection and subsequently decreased, whereas the cortex/cerebellum ratio was 1.3. The peak level (0.02% injected dose/ml) was reached in the thalamus at 7 min. [^18^F]Nifene radioactivity was cleared out rapidly in all brain regions. Ding et al. (8) reported that the thalamus/cerebellum distribution volume ratio in a baboon study was higher for 6-[^18^F]FA (2.5–3.5) than for 2-[^18^F]FA (1.9–2.1) at 180 min. Therefore, [^18^F]nifene exhibited faster binding kinetics than 2-[^18^F]FA and 6-[^18^F]FA.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Kimes A.S., Horti A.G., London E.D., Chefer S.I., Contoreggi C., Ernst M., Friello P., Koren A.O., Kurian V., Matochik J.A., Pavlova O., Vaupel D.B., Mukhin A.G. (2003). 2-[18F]F-A-85380: PET imaging of brain nicotinic acetylcholine receptors and whole body distribution in humans. Faseb J.
5 Ding Y., Liu N., Wang T., Marecek J., Garza V., Ojima I., Fowler J.S. (2000). Synthesis and evaluation of 6-[(18)F]fluoro-3-(2(S)-azetidinylmethoxy)pyridine as a PET tracer for nicotinic acetylcholine receptors. Nucl Med Biol.
6 Pichika R., Easwaramoorthy B., Collins D., Christian B.T., Shi B., Narayanan T.K., Potkin S.G., Mukherjee J. (2006). Nicotinic alpha4beta2 receptor imaging agents: part II. Synthesis and biological evaluation of 2-[18F]fluoro-3-[2-((S)-3-pyrrolinyl)methoxy]pyridine (18F-nifene) in rodents and imaging by PET in nonhuman primate. Nucl Med Biol.
7 Easwaramoorthy B., Pichika R., Collins D., Potkin S.G., Leslie F.M., Mukherjee J. (2007). Effect of acetylcholinesterase inhibitors on the binding of nicotinic alpha4beta2 receptor PET radiotracer, (18)F-nifene: A measure of acetylcholine competition. Synapse.
8 Ding Y.S., Fowler J.S., Logan J., Wang G.J., Telang F., Garza V., Biegon A., Pareto D., Rooney W., Shea C., Alexoff D., Volkow N.D., Vocci F. (2004). 6-[18F]Fluoro-A-85380, a new PET tracer for the nicotinic acetylcholine receptor: studies in the human brain and in vivo demonstration of specific binding in white matter. Synapse.